# 2-[^11^C]Methyl-6-(2-phenylethynyl)pyridine

Chemical name: | 2-[^11^C]Methyl-6-(2-phenylethynyl)pyridine
Abbreviated name: | [^11^C]MPEP
Synonym:
Agent Category: | Compound
Target: | Metabotropic glutamate subtype 5 (mGlu5) receptor (mGluR5 or mGluR_5_)
Target Category: | Receptor binding
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=metabotropic+glutamate+receptor+subtype+5+PET+ligand)]

2-[^11^C]Methyl-6-(2-phenylethynyl)pyridine ([^11^C]MPEP) is a radioligand developed for positron emission tomography (PET) imaging of metabotropic glutamate (mGlu) receptor subtype 5 (mGluR5 or mGluR_5_) in the central nervous system (CNS) (1). ^11^C is a positron emitter with a physical half-life (t_½_) of 20.3 min.

Glutamate is a major excitatory neurotransmitter at CNS synapses. Many neuroanatomical CNS projection pathways contain glutamatergic neurons (2). Glutamate produces its excitatory effects by acting on cell-surface ionotropic glutamate or mGluRs (3). The mGluRs are G-protein–coupled receptors, and the eight mGluR subtypes are further subdivided into groups I, II, and III. The group I receptors include mGluR1 and mGluR5, and they are found predominantly in postsynaptic locations. The mGluR5s are found with high to moderate density in the frontal cortex, caudate, putamen, nucleus accumbens, olfactory tubercle, hippocampus, and dorsal horn of the spinal cord, whereas the density in the cerebellum is low. These receptors are coupled to phospholipase C and up- or downregulate neuronal excitability. They have been implicated in a variety of diseases in the CNS, including anxiety, depression, schizophrenia, Parkinson’s disease, and drug addiction or withdrawal. These receptors are also involved in the modulation of various pain states, which makes them attractive targets for therapeutic drug development.

PET and single-photon emission computed tomography imaging of radioligands that target mGluR5s can be used to visualize and study the CNS mGluR5s in normal and pathological states. Some mGluR5 antagonists have been successfully labeled, but their in vivo visualization has been hampered by high lipophilicity, unfavorable brain uptake kinetics, or high metabolism (4, 5). MPEP and its methyl analog M-MPEP have been identified as potent and highly selective noncompetitive antagonists for mGlu5 (1, 6). Yu et al. (1) synthesized [^11^C]MPEP and demonstrated the feasibility of using it as a PET imaging ligand for in vivo imaging.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(metabotropic+glutamate+receptor+subtype+5+PET+ligand)+AND+synthesis)]

Yu et al. (1) reported the synthesis of [^11^C]MPEP from its stannyl precursor. The precursor was prepared from 2-bromo-6-(phenylethynyl)pyridine. Briefly, phenylacetylene was added to a mixture of 2,6-dibromopyridine, CuI, PdCl_2_(PPh_3_)_2_, and triethylamine. The mixture was stirred at room temperature for 27 h. The product was then filtered and purified on a silica gel column. The yield of 2-bromo-6-(phenylethynyl)pyridine was 42%. This was then reacted with tetrakis(triphenylphosphine)palladium(0) (Pd(0)) and toluene in a Chemglass cylindrical pressure vessel. A nitrogen stream was bubbled through the solution, and hexamethyldistannane was added. The pressure vessel was then capped and heated to 115–120ºC for 6 h. After filtration on a silica gel column, the residue was stirred for 2 h with saturated aqueous sodium bicarbonate and 35% aqueous hydrogen peroxide to oxidize PPh_3_ to PPh_3_O for removal by column chromatography. The yield of the MPEP precursor, 2-(trimethylstannyl)-6-(2-phenylethynyl)pyridine, was 51%. For the radiosynthesis, [^11^C]carbon dioxide ([^11^C]CO_2_) was produced by the ^14^N(p, α)^11^C nuclear reaction in nitrogen, and [^11^C]CO_2_ was transformed to [^11^C]methyl iodide ([^11^C]CH_3_I) for radiolabeling. The MPEP precursor was reacted with [^11^C]CH_3_I by the rapid Stille coupling reaction of aromatic stannanes. In this reaction, Pd(0) was used as the catalyst in toluene, and the reaction mixture was heated for 5 min at 100ºC. The radiochemical purity was 97.4 ± 2.3% (n = 14), and the specific activity was 40.4 ± 5.0 GBq/μmol (1,093 ± 134 mCi/μmol). The radiochemical yield was 12.6 ± 10.6 mCi at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(metabotropic+glutamate+receptor+subtype+5+PET+ligand)+AND+in+vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(metabotropic+glutamate+receptor+subtype+5+PET+ligand)+AND+rodentia)]

PET imaging was performed in male rats (1). Each anesthetized rat received 92.91 ± 34.15 MBq (2.51 ± 0.92 mCi) in 0.433 ± 0.163 μg ((2–3 nM)/0.1 ml or 2.3 nmol calculated from the mean specific activity of 1.09 mCi/nmol) by i.v. administration. Imaging showed high and rapid radioactivity accumulation of [^11^C]MPEP in brain areas, including the olfactory bulb, striatum, hippocampus, frontal cortex, and cerebellum. The maximum accumulation occurred in 2–3 min except in the olfactory bulb, where the radioactivity accumulated up to 10 min. The highest accumulation was in the olfactory area, followed by the hippocampus, cortex, and striatum. The radioactivity level ratio of olfactory bulb/cerebellum reached the maximum of 7.0 at 30 min. The radioactivity levels (n = 9) of the whole brain in percentage of the injected dose per cubic centimeter (% ID/cc) obtained from volumetric region-of-interest image analysis were 0.402 ± 0.066 (5 min), 0.223 ± 0.031 (10 min), 0.159 ± 0.018 (20 min), 0.128 ± 0.012 (30 min), 0.112 ± 0.009 (40 min), 0.096 ± 0.053 (50 min), and 0.094 ± 0.048 (60 min). The radioactivity levels (% ID/cc) of the olfactory bulb were 1.060 ± 0.182 (5 min), 1.110 ± 0.040 (10 min), 0.954 ± 0.032 (20 min), 0.821 ± 0.041 (30 min), 0.724 ± 0.058 (40 min), 0.616 ± 0.036 (50 min), and 0.568 ± 0.315 (60 min). When a blocking dose of 10 mg/kg unlabeled MPEP was administered 5 min before the radioligand injection (102.601 ± 18.06 MBq (2.77 ± 0.49 mCi) or 0.490 ± 0.079 μg (2.53 nmol calculated from the mean specific activity of 1.093 mCi/nmol)), the radioactivity levels (n = 4) of the olfactory lobe were decreased by 45.1% at 5 min and 61.5% at 40 min. High radioactivity levels were also observed in the liver, pancreas, and intestine. With the blocking dose of MPEP, the radioactivity levels (%ID/cc) of the duodenum (n = 2) decreased from 0.299 ± 0.083 to 0.131 ± 0.077 at 20 min and from 0.379 ± 0.074 to 0.079 ± 0.038 at 60 min. In another study that used a higher blocking dose at an earlier time point (MPEP 20 mg/kg at 10 s before radioligand injection) in two rats, there was decreased accumulation in all brain areas until 40 min. The radioactivity level decreases in the olfactory area were 80.2 ± 14.5% and 80.0 ± 8.2% at 5 min and 40 min, respectively. In the striatal area, the decreases were 35.8 ± 20.5% and 16.5 ± 14.0% at 5 min and 40 min, respectively.

In the in vivo metabolism study, [^11^C]MPEP was shown by high-performance liquid chromatography analysis to be rapidly metabolized after administration (1). The percentage of the radioligand remaining intact in the plasma after administration (n = 2) was 26.2 ± 6.2% at 5 min and 3.5 ± 2.6% at 20 min. No any lipophilic metabolite from [^11^C]MPEP was found.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(metabotropic+glutamate+receptor+subtype+5+PET+ligand)+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(metabotropic+glutamate+receptor+subtype+5+PET+ligand)+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(metabotropic+glutamate+receptor+subtype+5+PET+ligand)+AND+human)]

No publication is currently available.

## NIH Support

NIH/NIBIB grant EB01850.

## References

1 Yu M., Tueckmantel W., Wang X., Zhu A., Kozikowski A.P., Brownell A.L. (2005). Methoxyphenylethynyl, methoxypyridylethynyl and phenylethynyl derivatives of pyridine: synthesis, radiolabeling and evaluation of new PET ligands for metabotropic glutamate subtype 5 receptors. Nucl Med Biol.
2 Pin J.P., Duvoisin R. (1995). The metabotropic glutamate receptors: structure and functions. Neuropharmacology.
3 Slassi A., Isaac M., Edwards L., Minidis A., Wensbo D., Mattsson J., Nilsson K., Raboisson P., McLeod D., Stormann T.M., Hammerland L.G., Johnson E. (2005). Recent advances in non-competitive mGlu5 receptor antagonists and their potential therapeutic applications. Curr Top Med Chem.
4 Ametamey S.M., Kessler L.J., Honer M., Wyss M.T., Buck A., Hintermann S., Auberson Y.P., Gasparini F., Schubiger P.A. (2006). Radiosynthesis and Preclinical Evaluation of 11C-ABP688 as a Probe for Imaging the Metabotropic Glutamate Receptor Subtype 5. J Nucl Med.
5 Patel S., Ndubizu O., Hamill T., Chaudhary A., Burns H.D., Hargreaves R., Gibson R.E. (2005). Screening cascade and development of potential Positron Emission Tomography radiotracers for mGluR5: in vitro and in vivo characterization. Mol Imaging Biol.
6 Gasparini F., Andres H., Flor P.J., Heinrich M., Inderbitzin W., Lingenhohl K., Muller H., Munk V.C., Omilusik K., Stierlin C., Stoehr N., Vranesic I., Kuhn R. (2002). [(3)H]-M-MPEP, a potent, subtype-selective radioligand for the metabotropic glutamate receptor subtype 5. Bioorg Med Chem Lett.